# 18-[^18^F]Fluoro-4-thia-oleate

Chemical name: | 18-[^18^F]Fluoro-4-thia-oleate
Abbreviated name: | [^18^F]FTO
Synonym:
Agent category: | Compound
Target: | Fatty acid oxidation (FAO) enzymes
Target category: | Enzyme
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20FTO)]

β-Oxidation of long-chain fatty acids is the major (60%–80%) aerobic process for energy production in the heart, liver, and skeletal muscle. Abnormalities of fatty acid oxidation (FAO) are associated with several cardiovascular diseases, neurodegeneration, fatty liver, and diabetes (1-5). Myocardium has a high mitochondrial content because of high energy usage. Carnitine palmitoyltransferases (CPT1 and CPT2) mediate transfer of fatty acids into the mitochondrial matrix for β-oxidation (6, 7). Various radiolabeled, thia-substituted, fatty acid analogs have been found to be metabolically trapped in the myocardial mitochondria (8-10). 4-Thia fatty acids are oxidized in the mitochondria to 4-thia-enoyl-CoAs, which cannot be further metabolized and trapped (protein-bound) in the mitochondria. Oleate (18:1) is preferentially oxidized relative to palmitate (16:0) and stearate (18:0) by the mitochondrial FAO (11). DeGrado et al. (12) have synthesized 18-[^18^F]fluoro-4-thia-oleate ([^18^F]FTO) for evaluation as a positron emission tomography (PET) agent of FAO.

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=Fatty%20acid%20oxidation%20AND+micad%5Bbook%5D)
- Gene information in NCBI (CPT1 (http://www.ncbi.nlm.nih.gov/gene/1374))
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/omim/600528)
- Clinical trials (CPT1 (http://www.clinicaltrials.gov/ct2/results?term=Carnitine+palmitoyltransferase))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20FTO+synthesis)]

[^18^F]FTO was prepared as described by DeGrado et al. (12). [^18^F]Fluoride/Kryptofix 2.2.2/K_2_CO_3_ and the bromoester precursor ((Z)-methyl-18-bromo-4-thia-octadec-9-enoate) were heated in acetonitrile for 15 min at 75°C, followed by hydrolysis with KOH for 4 min at 90°C. [^18^F]FTO was purified with high-performance liquid chromatography with radiochemical yields of 20%–30% and a radiochemical purity of >99%. Specific activity of [^18^F]FTO was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20FTO%20and%20in%20vitro)]

No publication is currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20FTO%20and%20rodentia)]

DeGrado et al. (12) performed ex vivo biodistribution studies of [^18^F]FTO in rats. [^18^F]FTO accumulated mainly in the liver and heart with 0.70 ± 0.30% injected dose/g (ID/g) and 1.19 ± 0.16% ID/g, respectively, at 30 min after injection. Retention of [^18^F]FTO in the heart at 120 min was good with 0.82 ± 0.23% ID/g, whereas there was a slight washout in the liver (0.85 ± 0.22% ID/g). Pretreatment with the CPT1 inhibitor etomoxir (40 mg/kg, 120 min before [^18^F]FTO injection) reduced the radioactivity level in the heart by 82% at 30 min after injection with only 28% reduction in the liver. Folch-type analysis of the excised hearts showed that 90% of [^18^F]FTO radioactivity was protein-bound. Pretreatment with etomoxir reduced the protein-bound radioactivity to 24%. The heart/blood, heart/lung, heart/brain, and heart/muscle ratios were 44, 36, 37, and 48, respectively, at 120 min after injection. The uptake in the bone was 0.15% ID/g at 30 min and 0.46% ID/g at 120 min, indicating some defluorination of [^18^F]FTO. Whole-body PET imaging showed that [^18^F]FTO accumulated mainly in the heart and liver, with low accumulation in the lung. Good myocardial images were observed at 55–115 min after injection with little interference from the lung and liver. Some bone uptake was observed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F%20FTO+and+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20FTO%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20FTO%20and%20human)]

No publication is currently available.

## NIH Support

R01 HL63371, R01 CA108620

## References

1 Stanley W.C., Recchia F.A., Lopaschuk G.D. (2005). Myocardial substrate metabolism in the normal and failing heart. Physiol Rev.
2 Bergmann S.R., Herrero P., Sciacca R., Hartman J.J., Rubin P.J., Hickey K.T., Epstein S., Kelly D.P. (2001). Characterization of altered myocardial fatty acid metabolism in patients with inherited cardiomyopathy. J Inherit Metab Dis.
3 Liu Y. (2006). Fatty acid oxidation is a dominant bioenergetic pathway in prostate cancer. Prostate Cancer Prostatic Dis.
4 You M., Crabb D.W. (2004). Recent advances in alcoholic liver disease II. Minireview: molecular mechanisms of alcoholic fatty liver. Am J Physiol Gastrointest Liver Physiol.
5 Stanley W.C., Lopaschuk G.D., McCormack J.G. (1997). Regulation of energy substrate metabolism in the diabetic heart. Cardiovasc Res.
6 Jogl G., Hsiao Y.S., Tong L. (2004). Structure and function of carnitine acyltransferases. Ann N Y Acad Sci.
7 Bonnefont J.P., Djouadi F., Prip-Buus C., Gobin S., Munnich A., Bastin J. (2004). Carnitine palmitoyltransferases 1 and 2: biochemical, molecular and medical aspects. Mol Aspects Med.
8 Taylor M., Wallhaus T.R., Degrado T.R., Russell D.C., Stanko P., Nickles R.J., Stone C.K. (2001). An evaluation of myocardial fatty acid and glucose uptake using PET with [18F]fluoro-6-thia-heptadecanoic acid and [18F]FDG in Patients with Congestive Heart Failure. J Nucl Med.
9 DeGrado T.R., Wang S., Rockey D.C. (2000). Preliminary evaluation of 15-[18F]fluoro-3-oxa-pentadecanoate as a PET tracer of hepatic fatty acid oxidation. J Nucl Med.
10 Stone C.K., Pooley R.A., DeGrado T.R., Renstrom B., Nickles R.J., Nellis S.H., Liedtke A.J., Holden J.E. (1998). Myocardial uptake of the fatty acid analog 14-fluorine-18-fluoro-6-thia-heptadecanoic acid in comparison to beta-oxidation rates by tritiated palmitate. J Nucl Med.
11 DeLany J.P., Windhauser M.M., Champagne C.M., Bray G.A. (2000). Differential oxidation of individual dietary fatty acids in humans. Am J Clin Nutr.
12 DeGrado T.R., Bhattacharyya F., Pandey M.K., Belanger A.P., Wang S. (2010). Synthesis and preliminary evaluation of 18-(18)F-fluoro-4-thia-oleate as a PET probe of fatty acid oxidation. J Nucl Med.